# (2-methoxy-^11^C)-N-(4-(3,4-Dihydro-6,7-dimethoxy-isoquinolin-2(1H)-yl)butyl)-5-methylbenzamide

Chemical name: | (2-methoxy-^11^C)-N-(4-(3,4-Dihydro-6,7-dimethoxy-isoquinolin-2(1H)-yl)butyl)-5-methylbenzamide
Abbreviated name:
Synonym: | [^11^C]RHM-1, [^11^C]2
Agent Category: | Compound
Target: | σ_2_ sigma receptors
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=sigma2%20and%20carbon%20radioisotopes)]

Sigma receptors are functional, membrane-bound proteins distributed in the central nervous system (CNS) and peripheral organs such as the liver, kidneys, and endocrine glands (1, 2). The CNS sigma receptors are unique binding sites related to higher brain function. There are at least two subtypes of sigma receptors, σ_1_ and σ_2_. These receptors appear to be involved in numerous pharmacologic and physiologic functions, and they also modulate a number of central neurotransmitter systems. Studies suggest that these receptors may play a role in the pathogenesis of psychiatric disorders (3, 4). The σ_1_ receptors appear to play a role in CNS disorders and motor functions. The σ_2_ receptors (linked to potassium channels and calcium release) are also implicated in malignant neoplastic diseases (5-7). The density of σ_2_ receptors was found to be greater than that of σ_1_ receptors in tumor cells. For example, the density of σ_2_ receptors was found to be 10-fold higher in proliferating versus quiescent mouse mammary adenocarcinoma cells. Furthermore, it has been observed that σ_2_ receptor ligands can induce apoptosis in tumor cells. Because of these effects, sigma receptor ligands may be useful for detection and treatment in neurology and oncology.

N-[4-(3,4-Dihydro-6,7-dimethoxyisoquinolin-2(1H)-yl)butyl]-2-methoxy-5-methyl-benzamide (RHM-1) and N-[2-(3,4-dihydro-6,7-dimethoxyisoquinolin-2(1H)-yl)ethyl]-2-methoxy-5-methylbenzamide (RHM-2), two conformationally flexible benzamide analogs, have been shown to have a high affinity (K_i_ < 15 nM) and selectivity (σ_2_/σ_1_ ratio > 300) for σ_2_ receptors (8). The 2-methoxy group of RHM-1 and RHM-2 was used to introduce the ^11^C-labeled methyl group via O-alkylation of the corresponding phenol precursor. [^11^C]RHM-1 has been evaluated as a PET agent for imaging breast tumors in mice (9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=sigma2%20and%20carbon%20radioisotopes%20and%20synthesis)]

[^11^C]RHM-1 was synthesized by O-alkylation of the desmethyl compound, N-[2-(6,7-dimethoxy-3,4-dihydro-1H-isoquinolin-2-yl)-butyl]-2-hydroxy-5-methyl-benzamide, with [^11^C]methyl iodide (9). Reaction in NaOH/DMF with subsequent chromatographic separation gave radiochemical yields of 60–75%, with a total synthesis time of 50–60 min and a radiochemical purity >95%. The average specific activity was 148 GBq/μmol (4 Ci/μmol) at the end of bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=sigma2%20and%20carbon%20radioisotopes%20and%20in%20vitro)]

RHM-1 has been reported to have selective binding affinity to σ_2_ receptor sites in homogenates of rat liver membranes (8). The K_i_ values for σ_2_ and σ_1_ were 10.3 ± 1.5 and 3,078 ± 87 nM, respectively. The affinity of RHM-1 for the σ_2_ receptors is about 300-fold lower than that for the σ_1_ receptors. Xu et al. (10) reported that [^3^H]RHM-1 had a higher affinity [dissociation constant (K_d_) = 0.66 nM] for σ_2_ receptors than [^3^H]RHM-2 (K_d_ = 19.48 nM). The [^3^H]RHM-1 σ_2_ receptor densities (B_max_) for rat liver, MDA-MB human breast tumors, and EMT mouse breast tumors were found to be 1,099 ± 67, 1,820 ± 70, and 2,290 ± 30 fmol/mg protein, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=sigma2%20and%20carbon%20radioisotopes%20and%20rodentia)]

Tu et al. (9) performed biodistribution studies in EMT-6 tumor-bearing mice. Their studies showed the highest accumulation of radioactivity in the tumors with [^11^C]RHM-1 compared with three other ^11^C-labeled RHM-1 analogs. Tumor accumulation of [^11^C]RHM-1 was 4.22% injected dose (% ID)/g at 5 min, 2.35% ID/g at 30 min, and 1.32% ID/g at 60 min after injection. The liver and kidneys showed higher uptake than the tumors with a rapid clearance. Coinjection of [^11^C]RHM-1 with 1 mg/kg YUN 143 (a σ_2_ and σ_1_ high-affinity ligand) decreased the tumor/blood, tumor/lung, tumor/muscle, and tumor/fat ratios by 18–46% at 30 min. A study was also conducted comparing the tumor uptake and tumor/tissue ratios of [^11^C]RHM-1 against 3'-deoxy-3'-[^18^F]fluorothymidine ([^18^F]FLT), a radiolabeled nucleoside analog for measuring tumor proliferation. It was found that [^18^F]FLT had a higher tumor uptake (approximately 5.75% ID/g) than [^11^C]RHM-1 (approximately 2.25% ID/g) at 30 min. However, [^11^C]RHM-1 had either similar (lung, fat) or better (blood, muscle) tumor/tissue ratios than [^18^F]FLT in the tissues that are important for breast tumor imaging.

### Other Non-Primate Mammals

[PubMed]

No relevant publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=sigma2%20and%20carbon%20radioisotopes%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=sigma2%20and%20carbon%20radioisotopes%20and%20human)]

No publication is currently available.

## NIH Support

CA 102869

## References

1 Bowen W.D. (2000). Sigma receptors: recent advances and new clinical potentials. Pharm Acta Helv.
2 Walker J.M., Bowen W.D., Walker F.O., Matsumoto R.R., De Costa B., Rice K.C. (1990). Sigma receptors: biology and function. Pharmacol Rev.
3 Mishina M., Ishiwata K., Ishii K., Kitamura S., Kimura Y., Kawamura K., Oda K., Sasaki T., Sakayori O., Hamamoto M., Kobayashi S., Katayama Y. (2005). Function of sigma1 receptors in Parkinson's disease. Acta Neurol Scand.
4 Skuza G., Wedzony K. (2004). Behavioral pharmacology of sigma-ligands. Pharmacopsychiatry.
5 Colabufo N.A., Berardi F., Contino M., Ferorelli S., Niso M., Perrone R., Pagliarulo A., Saponaro P., Pagliarulo V. (2006). Correlation between sigma2 receptor protein expression and histopathologic grade in human bladder cancer. Cancer Lett.
6 Vilner B.J., John C.S., Bowen W.D. (1995). Sigma-1 and sigma-2 receptors are expressed in a wide variety of human and rodent tumor cell lines. Cancer Res.
7 Wheeler K.T., Wang L.M., Wallen C.A., Childers S.R., Cline J.M., Keng P.C., Mach R.H. (2000). Sigma-2 receptors as a biomarker of proliferation in solid tumours. Br J Cancer.
8 Mach R.H., Huang Y., Freeman R.A., Wu L., Vangveravong S., Luedtke R.R. (2004). Conformationally-flexible benzamide analogues as dopamine D3 and sigma 2 receptor ligands. Bioorg Med Chem Lett.
9 Tu Z., Dence C.S., Ponde D.E., Jones L., Wheeler K.T., Welch M.J., Mach R.H. (2005). Carbon-11 labeled sigma2 receptor ligands for imaging breast cancer. Nucl Med Biol.
10 Xu J., Tu Z., Jones L.A., Vangveravong S., Wheeler K.T., Mach R.H. (2005). [3H]N-[4-(3,4-dihydro-6,7-dimethoxyisoquinolin-2(1H)-yl)butyl]-2-methoxy-5 -methylbenzamide: a novel sigma-2 receptor probe. Eur J Pharmacol.